# 8-[^123^I]Iodo-L-1,2,3,4-tetrahydro-7-hydroxyisoquinoline-3-carboxylic acid

Chemical name: | 8-[^123^I]iodo- L-1,2,3,4-tetrahydro-7-hydroxyisoquinoline-3-carboxylic acid
Abbreviated name: | [^123^I]ITIC, [^123^I]ITIC(OH)
Synonym:
Agent category: | Compound
Target: | Amino acid transporter T system and membrane potential
Target category: | Transporter
Method of detection: | SPECT, gamma planar
Source of signal: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20ITIC)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain (3). These amino acids are composed of naturally occurring amino acids, such as L-[^11^C]leucine, L-[^11^C]methionine ([^11^C]MET), and L-[^11^C]tyrosine, and non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. There are also ^123^I-labeled amino acids, such as L-phenylalanine and L-tyrosine, which are used in imaging in oncology (1, 4, 5).

To date, 20 amino acid transporter systems have been identified (1). Most of the amino acids are taken up by tumor cells not only through the Na^+^-independent L, T, and ASC transporter systems but also by the Na^+^-dependent A and B^0^ transporter systems (6). These amino acids are retained in tumor cells because of their higher metabolic activities than most normal cells (1). Malignant transformation increases the use of amino acids for energy, protein synthesis, and cell division. Tumor cells often overexpress in the transporter systems (7). L-[^11^C]MET, [^18^F]fluoro- L-m-tyrosine, L-[^11^C]leucine, and [^18^F]fluoro-α-methyl tyrosine have been widely used in the detection of tumors (2, 6) because they are moved into cells by various amino acid transporters and are incorporated into proteins. The fraction of radiolabeled amino acid incorporated into proteins is usually small compared with the total amount taken up into the cell in vitro. Recently, it was reported that 75% of L-[^11^C]leucine was incorporated into proteins of monkey brains at 60 min after injection of the tracer as measured by biochemical analysis and PET imaging (8). These natural amino acid imaging scans are based on amino acid transport and protein incorporation.

No non-natural amino acids are incorporated into proteins (2, 9). These amino acids are rapidly transported into tumor cells. They are retained inside the tumor cells because of their high cellular metabolism and their high activity of the amino acid transporters. Recently, new L-tyrosine analogs, such as O-(2-[^18^F]fluoroethyl)-L-tyrosine ([^18^F]FET), were synthesized and evaluated as amino acid PET tracers for the detection of brain tumors with a higher specificity as compared with [^18^F]fluoro-2-deoxy-2-D-glucose ([^18^F]FDG). 8-[^123^I]Iodo- L-1,2,3,4-tetrahydro-7-hydroxyisoquinoline-3-carboxylic acid ([^123^I]ITIC) is a cyclic analog of L-tyrosine. It accumulated moderately in human pancreatic carcinoma and glioblastoma cells but markedly in human prostate tumor cells, with only a marginal incorporation into proteins (10-13). The cellular uptake into the prostate tumor cells was not dependent on most amino acid transport systems but tentatively dependent on the membrane potential and amino acid transporter T system. [^123^I]ITIC is being developed as a single-photon emission computed tomography (SPECT) imaging agent of human prostate cancer.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20ITIC%20and%20synthesis)]

[^123^I]ITIC was synthesized by iodide oxidation of L-1,2,3,4-tetrahydro-7-hydroxyisoquinoline-3-carboxylic acid (TIC) with sodium ^123^I-labeled iodide in the presence of 1,3,4,6-tetrachloro-3α,6α-diphenylglycouril (Iodogen) as an oxidant for 5 min at room temperature (12). With a total synthesis time of 30 min, this one-step synthesis produced [^123^I]ITIC with a radiochemical yield of 80 ± 15% and a radiochemical purity of >98% after high-performance liquid chromatography. The specific activity was >1.5 GBq/μmol (41 mCi/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20ITIC%20and%20in%20vitro)]

[^123^I]ITIC showed a quickly increasing uptake into human T98 glioma, PaCa44 pancreas, PC-3 prostate, and DU-145 prostate tumor cells in the first 5 min in culture, followed by a plateau of nearly constant radioactivity until 90–120 min of incubation (10, 13). The uptake into the two prostate tumor cells (35–58% of the total loaded radioactivity) was much higher than the T98 and PaCa44 tumor cells (10–33% of the total loaded radioactivity). No significant incorporation of [^123^I]ITIC into proteins was detected. Testing with various amino acid transporter inhibitors in the two prostate tumor cell lines indicates that [^123^I]ITIC was not taken up by the common neutral amino acid carrier systems. The cellular uptake was dependent on the membrane potential because high K^+^ buffer stimulated the uptake. However, the cellular uptake was inhibited by L-tryptophan but not by L-tyrosine, which indicates a possible involvement of the T transporter system.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20ITIC%20and%20rodentia)]

Samnick et al. (13) reported biodistribution studies in rats bearing C6 glioma cells in the brain, which showed a high uptake of radioactivity in the kidneys [8.2% injected dose (ID)/g] at 15 min after injection of [^123^I]ITIC. Normal brain (0.07% ID/g) and the C6 tumor (0.27% ID/g) showed low uptakes of the tracer. The uptake in the C6 tumor was only 0.1% ID/g at 30–60 min compared with 0.05% ID/g in the normal brain. Therefore, [^123^I]ITIC was found to be unsuitable for detection of glioma cancer.

The biodistribution of [^123^I]ITIC was determined in CD-1 nu/nu mice transplanted with human PC-3 and DU-145 prostate cancer cells in the flank or orthotopically in the prostate (11). [^123^I]ITIC accumulated highly and specifically in the tumors, reaching 13.6 ± 2.1% to 16.2 ± 2.5% ID/g in the heterotopic tumors compared with 14.8 ± 2.6% and 17.6 ± 3.4% ID/g in the orthotopic tumors at 60 and 240 min after injection, respectively. In contrast, accumulation of radioactivity in the blood, spleen, liver, and intestine was moderate and decreased with time, resulting in marked tumor/background ratios and excellent SPECT visualization of the tumors. Pretreatment of tumor-bearing mice with ITIC (1 mmol) 5 min before [^123^I]ITIC injection resulted in significant reduction in accumulation of radioactivity in the tumors (up to 70%) and kidneys (40–55%) at 240 min after injection, while the accumulation of [^123^I]ITIC in the blood, spleen, stomach, intestine, and liver was only marginally affected. Moreover, co-injection of [^123^I]ITIC with L-tyrosine (1 mmol) did not affect tissue and tumor accumulation. In contrast, co-injection of [^123^I]ITIC with L-tryptophan (1 mmol) inhibited radioactivity accumulation in the tumor (~40%), which supports possible involvement of the transporter T system. After injection of [^123^I]ITIC in the mice, 55–65% of the total radioactivity in the urine at 240 min was intact parent compound. Besides iodide (<10%), the main radioactive metabolite was more hydrophilic than [^123^I]ITIC. In a model of inflamed muscles in mice, the accumulation of [^123^I]ITIC in the inflamed muscles was similar to that of the healthy muscles. Therefore, [^123^I]ITIC did not accumulate significantly in the inflamed tissues.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20ITIC%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20ITIC%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=123I%20ITIC%20and%20human)]

No publication is currently available.

## References

1 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
2 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
3 Herholz K., Lercher M., Wienhard K., Bauer B., Lenz O., Heiss W.D. (2001). PET measurement of cerebral acetylcholine esterase activity without blood sampling. Eur J Nucl Med.
4 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
5 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
6 Langen K.J., Jarosch M., Muhlensiepen H., Hamacher K., Broer S., Jansen P., Zilles K., Coenen H.H. (2003). Comparison of fluorotyrosines and methionine uptake in F98 rat gliomas. Nucl Med Biol.
7 Saier M.H., Daniels G.A., Boerner P., Lin J. (1988). Neutral amino acid transport systems in animal cells: potential targets of oncogene action and regulators of cellular growth. J Membr Biol.
8 Smith C.B., Schmidt K.C., Qin M., Burlin T.V., Cook M.P., Kang J., Saunders R.C., Bacher J.D., Carson R.E., Channing M.A., Eckelman W.C., Herscovitch P., Laverman P., Vuong B.K. (2005). Measurement of regional rates of cerebral protein synthesis with L-[1-11C]leucine and PET with correction for recycling of tissue amino acids: II. Validation in rhesus monkeys. J Cereb Blood Flow Metab.
9 Wester H.J., Herz M., Weber W., Heiss P., Senekowitsch-Schmidtke R., Schwaiger M., Stocklin G. (1999). Synthesis and radiopharmacology of O-(2-[18F]fluoroethyl)-L-tyrosine for tumor imaging. J Nucl Med.
10 Samnick S., Fozing T., Kirsch C.M. (2006). Preparation and tumor affinity testing of the radioiodinated tetrahydroisoquinoline derivative [123I]TIC(OH) for targeting prostate cancer. Appl Radiat Isot.
11 Samnick S., Nestle U., Wagner M., Fozing T., Schaefer A., Menger M.D., Kirsch C.M. (2007). Validation of 8-[(123)I]iodo-l-1,2,3,4-tetrahydro-7-hydroxyisoquinoline-3-carboxylic acid as an imaging agent for prostate cancer in experimental models of human prostate cancer. Nucl Med Biol.
12 Samnick S., Richter S., Romeike B.F., Heimann A., Feiden W., Kempski O., Kirsch C.M. (2000). Investigation of iodine-123-labelled amino acid derivatives for imaging cerebral gliomas: uptake in human glioma cells and evaluation in stereotactically implanted C6 glioma rats. Eur J Nucl Med.
13 Samnick S., Schaefer A., Siebert S., Richter S., Vollmar B., Kirsch C.M. (2001). Preparation and investigation of tumor affinity, uptake kinetic and transport mechanism of iodine-123-labelled amino acid derivatives in human pancreatic carcinoma and glioblastoma cells. Nucl Med Biol.